# Microbubbles coated with antibody to mucosal addressin cellular adhesion molecule-1

Chemical name: | Microbubbles coated with antibody to mucosal addressin cellular adhesion molecule-1
Abbreviated name: | MB_MAdCAM-1_
Synonym:
Agent category: | Antibody
Target: | Mucosal addressin cellular adhesion molecule-1 (MAdCAM-1)
Target category: | Adhesion molecule
Method of detection: | Ultrasound (US)
Source of signal: | Microbubbles
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=2177172), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=109633021) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=8174) for more information about MAdCAM-1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20MAdCAM-1)]

Ultrasound is the most widely used imaging modality (1) and is expanding its role in noninvasive molecular imaging with ligand-carrying microbubbles (2). Microbubbles are comprised of spherical cavities filled by a gas encapsulated in a shell. The shells are made of phospholipids, surfactant, denatured human serum albumin or synthetic polymer. Ligands and antibodies can be incorporated into the shell surface of microbubbles. Microbubbles are usually 2 to 8 μm in size. They provide a strongly reflective interface and resonate to ultrasound waves. They are used as ultrasound contrast agents in imaging of inflammation, angiogenesis, intravascular thrombus, and tumors (3-5). They are also potentially used for drug and gene delivery (6).

Endothelial cells are important cells in inflammatory responses (7, 8). Bacterial lipopolysaccharide (LPS), virus, inflammation, and tissue injury increase tumor necrosis factor α (TNFα), interleukin-1 (IL-1) and other cytokine and chemokine secretion. Leukocyte emigration from blood is dependent on their rolling along endothelial cell surfaces and subsequently adherence to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell surface adhesion molecules, such as intracellular adhesion molecule-1 (ICAM-1), vascular cell adhesion molecule-1 (VCAM-1), integrins and selectins. Chemokines are chemotactic to leukocytes to sites of inflammation and tissue injury. The movements of leukocytes through endothelial junctions into the extravascular space are highly orchestrated through various interactions with different adhesion molecules on endothelial cells (9).

Mucosal addressin cellular adhesion molecule-1 (MAdCAM-1) is found on cell surface of endothelial cells in the mucosal lymphoid tissues, mesenteric lymph nodes, intestines and mammary gland (10, 11). It binds to α4β7 integrin receptors on the cell-surface of leukocytes (12). IL-1 and TNFα stimulate MAdCAM-1 expression on these endothelial cells (13). Inflammation leads to leukocyte adhesion to the activated endothelium. It has been shown that MAdCAM-1 expression is up-regulated in humans with active ulcerative colitis and Crohn’s disease (14). Microbubbles targeted with antibody against MAdCAM-1 are being developed as a noninvasive agent for MAdCAM-1 expression in vascular endothelial cells of dysfunctional endothelium (15).

### Related Resource Links:

- Chapters in MICAD (MAdCAM-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=MAdCAM-1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (MAdCAM-1 (http://www.ncbi.nlm.nih.gov/gene/8174))
- Articles in Online Mendelian Inheritance in Man (OMIM) (MAdCAM-1 (http://www.ncbi.nlm.nih.gov/omim/102670))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20MAdCAM-1%20and%20synthesis)]

For targeted microbubbles, Bachmann et al. (15) prepared biotinylated microbubbles by sonication of an aqueous dispersion of decafluorobutane gas, phosphatidylcholine, polyethyleneglycol-(PEG-)stearate, and distearoylphosphatidylethanolamine-PEG-biotin. Microbubbles were combined with streptavidin, washed, and conjugated with biotinylated mouse monoclonal antibody against MAdCAM-1 (MB_MAdCAM-1_) or isotype control monoclonal antibody (MB_iso_). The microbubbles are about 3.9 µm in diameter. An antibody to microbubble ratio was estimated to be ~100,000 by flow cytometry.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20MAdCAM-1%20and%20in%20vitro)]

Bachmann et al. (15) reported that MB_MAdCAM-1_ (5 x 10^5^/ml) perfused through the flow chamber coated with MAdCAM-1 at a wall shear rate of 0.5 dyne/cm^2^. There were >600 MB_MAdCAM-1_/mm^2^ and less than 10 MB_iso_/mm^2^. Pre-incubation with anti-MAdCAM-1 antibody prior to infusion of MB_MAdCAM-1_ decreased the binding of MB_MAdCAM-1_ to ~50 MB_MAdCAM-1_/mm^2^. There was a significantly greater number of MB_MAdCAM-1_ attached to TNF-activated endothelial cells (484 ± 50 microbubbles/mm^2^) than to normal endothelial cells (75 ± 19 microbubbles/mm^2^) in the flow chamber experiments. MB_iso_ attachment to activated and normal endothelial cells was 26 ± 3 and 11 ± 2 microbubbles/mm^2^, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20MAdCAM-1%20and%20rodentia)]

Bachmann et al. (15) performed ultrasound assessment of spontaneous ileal inflammation in SAMP mice as compared to normal AKR mice after injection of 5 X 10^6^ microbubbles. Transabdominal ultrasound imaging of inflamed ileal segments in SAMP mice (10 U ± 2, n = 14) showed that video intensity signal was significantly higher (P<0.01) than control non-inflamed segments in AKR mice (1 U ± 1, n = 6) for MB_MAdCAM-1_. On the other hand, control MB_iso_ exhibited a minimal contrast in both the SAMP (3 U ± 1, n = 14) and AKR (2 U ± 1, n = 6) ileal segments. Postmortem histology confirmed that the SAMP ileal segments had a significantly higher infiltration of inflammatory cells than the control ARK ileal segments. There was a strong positive correlation (R^2^ = 0.92) of video intensities with total inflammatory scores in SAMP mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20MAdCAM-1%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20MAdCAM-1%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20MAdCAM-1%20and%20human)]

No publication is currently available.

## NIH Support

P01 DK57880, P30 DK56703

## References

1 Wells P.N. (2001). Physics and engineering: milestones in medicine. Med Eng Phys.
2 Liang H.D., Blomley M.J. (2003). The role of ultrasound in molecular imaging. Br J Radiol.
3 Klibanov A.L. (2005). Ligand-carrying gas-filled microbubbles: ultrasound contrast agents for targeted molecular imaging. Bioconjug Chem.
4 Lindner J.R. (2004). Microbubbles in medical imaging: current applications and future directions. Nat Rev Drug Discov.
5 Villanueva F.S., Wagner W.R., Vannan M.A., Narula J. (2004). Targeted ultrasound imaging using microbubbles. Cardiol Clin.
6 Dijkmans P.A., Juffermans L.J., Musters R.J., van Wamel A., ten Cate F.J., van Gilst W., Visser C.A., de Jong N., Kamp O. (2004). Microbubbles and ultrasound: from diagnosis to therapy. Eur J Echocardiogr.
7 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
8 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
9 Vanderslice P., Woodside D.G. (2006). Integrin antagonists as therapeutics for inflammatory diseases. Expert Opin Investig Drugs.
10 Connor E.M., Eppihimer M.J., Morise Z., Granger D.N., Grisham M.B. (1999). Expression of mucosal addressin cell adhesion molecule-1 (MAdCAM-1) in acute and chronic inflammation. J Leukoc Biol.
11 Nakache M., Berg E.L., Streeter P.R., Butcher E.C. (1989). The mucosal vascular addressin is a tissue-specific endothelial cell adhesion molecule for circulating lymphocytes. Nature.
12 Berlin C., Berg E.L., Briskin M.J., Andrew D.P., Kilshaw P.J., Holzmann B., Weissman I.L., Hamann A., Butcher E.C. (1993). Alpha 4 beta 7 integrin mediates lymphocyte binding to the mucosal vascular addressin MAdCAM-1. Cell.
13 Ando T., Jordan P., Wang Y., Itoh M., Joh T., Sasaki M., Elrod J.W., Carpenter A., Jennings M.H., Minagar A., Alexander J.S. (2005). MAdCAM-1 expression and regulation in murine colonic endothelial cells in vitro. Inflamm Bowel Dis.
14 Arihiro S., Ohtani H., Suzuki M., Murata M., Ejima C., Oki M., Kinouchi Y., Fukushima K., Sasaki I., Nakamura S., Matsumoto T., Torii A., Toda G., Nagura H. (2002). Differential expression of mucosal addressin cell adhesion molecule-1 (MAdCAM-1) in ulcerative colitis and Crohn's disease. Pathol Int.
15 Bachmann C., Klibanov A.L., Olson T.S., Sonnenschein J.R., Rivera-Nieves J., Cominelli F., Ley K.F., Lindner J.R., Pizarro T.T. (2006). Targeting mucosal addressin cellular adhesion molecule (MAdCAM)-1 to noninvasively image experimental Crohn's disease. Gastroenterology.